# [^18^F]Fluoro-2-deoxy-2-D-glucose

Chemical name: | [^18^F]Fluoro-2-deoxy-2-D-glucose
Abbreviated name: | [^18^F]FDG, FDG
Synonym: | [^18^F]Fluorodeoxyglucose
Agent Category: | Compound
Target: | Glucose transporters and hexokinases
Target Category: | Transporters, enzymes
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorodeoxyglucose%20f18%22%5BMeSH%20Terms%5D)]

The phosphorylation of glucose, an initial and important step in cellular metabolism, is catalyzed by hexokinases (HKs) (1). There are four HKs in mammalian tissues. HKI, HKII, and HKIII have molecular weights of approximately 100,000 each. HKI is found mainly in the brain. HKII is insulin sensitive and found in adipose and muscle cells. HKIV, also known as glucokinase, has a molecular weight of 50,000 and is specific to the liver and pancreas. Most brain HK is bound to mitochondria, enabling coordination between glucose consumption and oxidation. Tumor cells are known to be highly glycolytic because of increased expression of glycolytic enzymes and HK activity (2), which was detected in tumors from patients with lung, gastrointestinal, and breast cancer. The HKs, by converting glucose to glucose-6-phosphate, help to maintain the downhill gradient that results in the transport of glucose into cells through the facilitative glucose transporters (GLUT1-13) (3). GLUT4 and HKII are the major transporter and HK isoform in skeletal muscle, heart, and adipose tissue, wherein insulin promotes glucose utilization. HKIV is associated with GLUT2 in liver and pancreatic β cells.

2-Deoxy-D-glucose (2DG) was first developed to inhibit glucose utilization by cancer cells (4). HKs phosphorylate 2DG to 2-DG-6-phosphate, which inhibits phosphorylation of glucose. 2-[^18^F]Fluoro-2-deoxy-D-glucose ([^18^F]FDG) was later developed for molecular imaging studies (5). FDG is moved into cells by glucose transporters and is then phosphorylated by HK to FDG-6- phosphate. FDG-6- phosphate cannot be metabolized further in the glycolytic pathway and stays intracellularly in the cells. Tumor cells do not contain a sufficient amount of glucose-6-phosphatase to reverse the phosphorylation. The elevated rates of glycolysis and glucose transport in many types of tumor cells and activated cells enhance the uptake of FDG in these cells relative to other normal cells. Positron emission tomography (PET) with [^18^F]FDG has been used to assess alternations in glucose metabolism in brain, cancer, cardiovascular diseases, Alzheimer’s disease and other central nervous system disorders, and infectious, autoimmune, and inflammatory diseases (6-11).

### Related Resource Links:

- Chapters in MICAD (Hexokinase (http://www.ncbi.nlm.nih.gov/books?term=(hexokinase%20OR%20hexokinases)%20AND%20micad%5Bbook%5D), glucose transporter (http://www.ncbi.nlm.nih.gov/books?term=glucose%20transporters%20%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Hexokinase (http://www.ncbi.nlm.nih.gov/gene?term=hexokinase%20human), Glut1 (http://www.ncbi.nlm.nih.gov/gene/6513)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (Hexokinase (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=hexokinase%5BAll+Fields%5D), Glut1 (http://www.ncbi.nlm.nih.gov/omim/138140))
- Clinical trials ([^18^F]FDG (http://www.clinicaltrials.gov/ct2/results?term=FDG))
- Drug information in FDA ([^18^F]FDG (http://google2.fda.gov/search?q=%5B18F%5DFDG&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=3&y=9))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Fluorodeoxyglucose%20F18%22%5BMeSH%5D%20AND%20%22chemical%20synthesis%22%5BSubheading%5D)]

[^18^F]FDG was synthesized by a direct electrophilic fluorination of 3,4,6-tri-O-acetyl-D-glucal with [^18^F]F_2_ gas with a radiochemical yield of 8% (12). [^18^F]FDG was also prepared by reacting ^18^F-labeled acetyl hypofluorite, prepared by reaction of ^18^F-labeled molecular fluorine with sodium acetate in glacial acetic acid, and tri-acetyl-D-glucal at room temperature. Overall radiochemical yield was about 24% with a radiochemical purity of 98%. The specific activity of [^18^F]FDG was about 25 GBq/mmol (685 mCi/mmol). The synthesis time was approximately 60 min (13). Subsequently, the radiochemical yields of [^18^F]FDG were improved to 50-60% by using various methods involving nucleophilic fluorination using fluoride of high specific activity (14-17). An automated synthesis of [^18^F]FDG using tetrabutylammonium [^18^F]fluoride was reported to give a radiochemical yield of 12-17% with 96-99% radiochemical purity (18).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorodeoxyglucose%20f18%22%5BMeSH%20Terms%5D%20AND%20in%20vitro)]

FDG and other glucose analogs were investigated as anticancer agents by inhibiting glycolysis of tumor cells grown in cell cultures. In vitro uptake studies of [^18^F]FDG by endothelial cells, monocytes, macrophages, neutrophils, granulocytes, lymphocytes, and tumor cells have been reported and shed some light on [^18^F]FDG uptake mechanisms in these cells (19-23). On the other hand, in organs such as the liver, FDG is taken up and rapidly released because of dephosphorylation by FDG-6-phosphatase (24). Therefore, the overall FDG uptake into cells is dependent on the activity of glucose transporters, HKs, and phosphatases.

Uptake of [^18^F]FDG in isolated human monocytes-macrophages (HMMs) in vitro was compared with that in human glioblastoma and pancreatic carcinoma cells (25). HMMs were cultured for 0, 7, and 14 days. [^18^F]FDG uptake in HMMs significantly increased with culture duration as monocytes differentiated into mature macrophages. The uptake of day 14 macrophages was similar to the two cancer cell lines. Lipopolysaccharide stimulation further enhanced [^18^F]FDG uptake in HMMs. [^18^F]FDG uptake significantly decreased with increasing glucose concentration in the medium. Radio-thin layer chromatography of intracellular metabolites revealed that [^18^F]FDG was trapped by HMMs mainly as [^18^F]FDG-6-phosphate and [^18^F]FDG-1,6-diphosphate. HMMs in tumors and inflamed tissues could result in high uptake of [^18^F]FDG.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorodeoxyglucose%20f18%22%5BMeSH%20Terms%5D%20AND%20rodentia%20NOT%20in%20vitro)]

[^18^F]FDG was accumulated rapidly into kidneys, liver, lung, and small intestine of normal mice, followed by a rapid clearance (26). On the other hand, the accumulation of the tracer in the brain and heart remained relatively constant during the 2 h of the experiment. [^18^F]FDG was tested as a tumor diagnostic agent in a transplantable rat tumor (27). Tissue distribution studies in rats showed high uptakes of [^18^F]FDG in the tumor, heart, intestine, and brain. Tumor uptake reached 2.65% dose [^18^F]FDG/g at 60 min and remained relatively constant until 120 min. Blood clearance [^18^F]FDG was very rapid, and tumor/blood ratios reached 22.1 at 60 min. Tumor/tissue ratios were very high in most organs, especially in the liver, kidneys, and pancreas.

Increased glucose metabolism of inflammatory tissues is the main source of false-positive [^18^F]FDG PET findings in oncology. The biodistribution of 3'-deoxy-3'-[^18^F]fluorothymidine [^18^F]FLT and [^18^F]FDG was studied in Wistar rats that bore tumors (C6 rat glioma in the right shoulder) and also had sterile inflammation in the left calf muscle (induced by injection of 0.1 ml of turpentine). Tumor/muscle ratios of [^18^F]FDG at 2 h after injection (13.2 ± 3.0) were higher than those of [^18^F]FLT (3.8 ± 1.3). [^18^F]FDG showed high uptake in brain and heart, whereas [^18^F]FLT showed high uptake in bone marrow. [^18^F]FDG was also accumulated in the inflamed muscle, with 4.8 ± 1.2 times higher uptake in the affected thigh than in the healthy thigh. In contrast to [^18^F]FLT, [^18^F]FDG uptake was not significantly different between the two thighs. In [^18^F]FDG PET images, both tumor and inflammation were visible, but [^18^F]FLT PET showed only the tumor (28).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorodeoxyglucose%20f18%22%5BMeSH%5D%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

There was an early and high uptake of [^18^F]FDG in a variety of transplantable tumors in mice, rats, hamsters, and rabbits (29). Tumor/blood and tumor/normal tissue ratios ranged from 2.6 to 17.8 and 2.1 to 9.2, respectively. Various [^18^F]FDG uptake studies were performed using dogs [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorodeoxyglucose%20f18%22%5BMeSH%20Terms%5D%20AND%20%28%22dogs%22%5BMeSH%20Terms%5D%20OR%20dogs%5BText%20Word%5D%29)], pigs [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorodeoxyglucose%20f18%22%5BMeSH%20Terms%5D%20AND%20%28%22swine%22%5BMeSH%20Terms%5D%20OR%20pigs%5BText%20Word%5D%29)], sheep [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorodeoxyglucose%20f18%22%5BMeSH%20Terms%5D%20AND%20%28%22sheep%22%5BMeSH%20Terms%5D%20OR%20sheep%5BText%20Word%5D%29)], and rabbits [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorodeoxyglucose%20f18%22%5BMeSH%20Terms%5D%20AND%20%28%22rabbits%22%5BMeSH%20Terms%5D%20OR%20rabbits%5BText%20Word%5D%29)].

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorodeoxyglucose%20f18%22%5BMeSH%20Terms%5D%20AND%20primate%20not%20human)]

Regional cerebral blood flow (rCBF) and regional cerebral metabolic rate of glucose (rCMRglc) were measured in old and young monkeys by PET. Studies were performed on six old and six young-adult male rhesus monkeys. rCBF and the rCMRglc were serially measured using PET with [^15^O]H_2_O and [^18^F]FDG, respectively. All PET emission scans were performed in the conscious state for the cerebellum, hippocampus, striatum, occipital cortex, temporal cortex, frontal cortex, and cingulate. Old monkeys had significantly lower rCBF in the cerebellum, hippocampus, striatum, occipital cortex, temporal cortex, and frontal cortex and significantly lower rCMRglc in the cerebellum, hippocampus, striatum, occipital cortex, temporal cortex, frontal cortex, and cingulate, compared with young monkeys (30).

Pathogenesis of simian immunodeficiency virus (SIV) infection in rhesus macaques begins with acute viremia and then progresses to a distributed infection in the solid lymphoid tissues. PET imaging with [^18^F]FDG from SIV-infected animals was distinguishable from uninfected controls and revealed a pattern consistent with widespread lymphoid tissue activation. Significant [^18^F]FDG accumulation in colon, along with mesenteric and ileocecal lymph nodes, was found in SIV infection, especially during terminal disease stages. Areas of elevated [^18^F]FDG uptake in the PET images were correlated with productive SIV infection. [^18^F]FDG PET images of SIV-infected animals correlated sites of virus replication with high FDG accumulation. Therefore, [^18^F]FDG can be used to evaluate the distribution and activity of infected tissues in a living animal without biopsy (31).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorodeoxyglucose%20f18%22%5BMeSH%20Terms%5D%20AND%20humans)]

In 1976, the first images of [^18^F]FDG metabolism in humans were obtained and showed the high uptake in the bladder, heart, and brain (5, 32). Regional kinetic constants and rCMRglc in normal human subjects were determined by [^18^F]FDG PET (33-36). Human dosimetry [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorodeoxyglucose%20f18%22%5BMeSH%20Terms%5D%20AND%20dosimetry%5BAll%20Fields%5D)] was estimated from absorbed dose in organs after intravenous administration of [^18^F]FDG using whole-body PET scans in six normal volunteers (37). The bladder received the highest dose of radioactivity, followed by the spleen, heart, and brain. Mejia et al (38) estimated the effective dose equivalent to be 0.024 mSv/MBq (81 mrem/mCi).

[^18^F]FDG PET imaging techniques are widely used in clinical applications. In central nervous system disorders [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorodeoxyglucose%20f18%22%5BMeSH%20Terms%5D%20AND%20%22humans%22%5BMeSH%20Terms%5D%20AND%20%22brain%22%5BMeSH%20Terms%5D)], the clinical applications are in Alzheimer’s disease, dementia, epilepsy, brain trauma, Huntington disease, cerebrovascular disorders, brain tumors, Schizophrenia, and mood disorders (39, 40). In oncology [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorodeoxyglucose%20f18%22%5BMeSH%20Terms%5D%20AND%20%28%22humans%22%5BMeSH%5D%20AND%20%22neoplasms%22%5BMeSH%20Terms%5D%29)], the clinical applications are in diagnosis, treatment monitoring, and tumor staging have been used in non-small cell lung cancer, colorectal carcinoma, malignant melanoma, Hodgkin and non-Hodgkin lymphoma, esophageal carcinoma, head and neck cancer, breast cancer, and thyroid carcinoma (9, 41). In cardiovascular disorders [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorodeoxyglucose%20f18%22%5BMeSH%20Terms%5D%20AND%20%22Humans%22%5BMeSH%5D%20AND%20%22cardiovascular%20system%22%5BMeSH%20Terms%5D)], the clinical applications are in myocardial viability and atherosclerosis (42). In infectious and inflammatory diseases [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluorodeoxyglucose%20f18%22%5BMeSH%20Terms%5D%20AND%20%22humans%22%5BMeSH%20Terms%5D%20AND%20%28%22inflammation%22%5BMeSH%5D%20OR%20%22infection%22%5BMeSH%20Terms%5D%29)], the clinical applications are in orthopedic infections, osteomyelitis, ileitis, sarcoidosis, rheumatologic disease, and vasculitis (42).

## References

1 Smith T.A. (2000). Mammalian hexokinases and their abnormal expression in cancer. Br J Biomed Sci.
2 Suolinna E.M., Haaparanta M., Paul R., Harkonen P., Solin O., Sipila H. (1986). Metabolism of 2-[18F]fluoro-2-deoxyglucose in tumor-bearing rats: chromatographic and enzymatic studies. Int J Rad Appl Instrum B.
3 Avril N. (2004). GLUT1 expression in tissue and (18)F-FDG uptake. J Nucl Med.
4 Laszlo J., Humphreys S.R., Goldin A. (1960). Effects of glucose analogues (2-deoxy-D-glucose, 2-deoxy-D-galactose) on experimental tumors. J Natl Cancer Inst.
5 Fowler J.S., Ido T. (2002). Initial and subsequent approach for the synthesis of 18FDG. Semin Nucl Med.
6 Phelps M.E. (2000). PET: the merging of biology and imaging into molecular imaging. J Nucl Med.
7 Phelps M.E., Mazziotta J.C. (1985). Positron emission tomography: human brain function and biochemistry. Science.
8 Phelps M.E., Mazziotta J.C., Huang S.C. (1982). Study of cerebral function with positron computed tomography. J Cereb Blood Flow Metab.
9 Rohren E.M., Turkington T.G., Coleman R.E. (2004). Clinical applications of PET in oncology. Radiology.
10 Sokoloff L. (1985). Basic principles in imaging of regional cerebral metabolic rates. Res Publ Assoc Res Nerv Ment Dis.
11 Spence A.M., Mankoff D.A., Muzi M. (2003). Positron emission tomography imaging of brain tumors. Neuroimaging Clin N Am.
12 Reivich M., Kuhl D., Wolf A., Greenberg J., Phelps M., Ido T., Casella V., Fowler J., Gallagher B., Hoffman E., Alavi A., Sokoloff L. (1977). Measurement of local cerebral glucose metabolism in man with 18F-2-fluoro-2-deoxy-d-glucose. Acta Neurol Scand Suppl.
13 Diksic M., Jolly D. (1983). New high-yield synthesis of 18F-labelled 2-deoxy-2-fluoro-D-glucose. Int J Appl Radiat Isot.
14 Mock B.H., Vavrek M.T., Mulholland G.K. (1996). Back-to-back "one-pot" [18F]FDG syntheses in a single Siemens-CTI chemistry process control unit. Nucl Med Biol.
15 Taylor M.D., Roberts A.D., Nickles R.J. (1996). Improving the yield of 2-[18F]fluoro-2-deoxyglucose using a microwave cavity. Nucl Med Biol.
16 Toorongian S.A., Mulholland G.K., Jewett D.M., Bachelor M.A., Kilbourn M.R. (1990). Routine production of 2-deoxy-2-[18F]fluoro-D-glucose by direct nucleophilic exchange on a quaternary 4-aminopyridinium resin. Int J Rad Appl Instrum B.
17 Hamacher K., Coenen H.H., Stocklin G. (1986). Efficient stereospecific synthesis of no-carrier-added 2-[18F]-fluoro-2-deoxy-D-glucose using aminopolyether supported nucleophilic substitution. J Nucl Med.
18 Brodack J.W., Dence C.S., Kilbourn M.R., Welch M.J. (1988). Robotic production of 2-deoxy-2-[18F]fluoro-D-glucose: a routine method of synthesis using tetrabutylammonium [18F]fluoride. Int J Rad Appl Instrum [A].
19 Deichen J.T., Schmidt C., Prante O., Maschauer S., Papadopoulos T., Kuwert T. (2004). Influence of TSH on uptake of [18F]fluorodeoxyglucose in human thyroid cells in vitro. Eur J Nucl Med Mol Imaging.
20 Smith T.A. (2001). The rate-limiting step for tumor [18F]fluoro-2-deoxy-D-glucose (FDG) incorporation. Nucl Med Biol.
21 Maschauer S., Prante O., Hoffmann M., Deichen J.T., Kuwert T. (2004). Characterization of 18F-FDG uptake in human endothelial cells in vitro. J Nucl Med.
22 Osman S., Danpure H.J. (1992). The use of 2-[18F]fluoro-2-deoxy-D-glucose as a potential in vitro agent for labelling human granulocytes for clinical studies by positron emission tomography. Int J Rad Appl Instrum B.
23 Vinals F., Gross A., Testar X., Palacin M., Rosen P., Zorzano A. (1999). High glucose concentrations inhibit glucose phosphorylation, but not glucose transport, in human endothelial cells. Biochim Biophys Acta.
24 Caraco C., Aloj L., Chen L.Y., Chou J.Y., Eckelman W.C. (2000). Cellular release of [18F]2-fluoro-2-deoxyglucose as a function of the glucose-6-phosphatase enzyme system. J Biol Chem.
25 Deichen J.T., Prante O., Gack M., Schmiedehausen K., Kuwert T. (2003). Uptake of [18F]fluorodeoxyglucose in human monocyte-macrophages in vitro. Eur J Nucl Med Mol Imaging.
26 Gallagher B.M., Ansari A., Atkins H., Casella V., Christman D.R., Fowler J.S., Ido T., MacGregor R.R., Som P., Wan C.N., Wolf A.P., Kuhl D.E., Reivich M. (1977). Radiopharmaceuticals XXVII. 18F-labeled 2-deoxy-2-fluoro-d-glucose as a radiopharmaceutical for measuring regional myocardial glucose metabolism in vivo: tissue distribution and imaging studies in animals. J Nucl Med.
27 Fukuda H., Matsuzawa T., Abe Y., Endo S., Yamada K., Kubota K., Hatazawa J., Sato T., Ito M., Takahashi T., Iwata R., Ido T. (1982). Experimental study for cancer diagnosis with positron-labeled fluorinated glucose analogs: [18F]-2-fluoro-2-deoxy-D-mannose: a new tracer for cancer detection. Eur J Nucl Med.
28 van Waarde A., Cobben D.C., Suurmeijer A.J., Maas B., Vaalburg W., de Vries E.F., Jager P.L., Hoekstra H.J., Elsinga P.H. (2004). Selectivity of 18F-FLT and 18F-FDG for differentiating tumor from inflammation in a rodent model. J Nucl Med.
29 Som P., Atkins H.L., Bandoypadhyay D., Fowler J.S., MacGregor R.R., Matsui K., Oster Z.H., Sacker D.F., Shiue C.Y., Turner H., Wan C.N., Wolf A.P., Zabinski S.V. (1980). A fluorinated glucose analog, 2-fluoro-2-deoxy-D-glucose (F-18): nontoxic tracer for rapid tumor detection. J Nucl Med.
30 Noda A., Ohba H., Kakiuchi T., Futatsubashi M., Tsukada H., Nishimura S. (2002). Age-related changes in cerebral blood flow and glucose metabolism in conscious rhesus monkeys. Brain Res.
31 Scharko A.M., Perlman S.B., Hinds P.W.n., Hanson J.M., Uno H., Pauza C.D. (1996). Whole body positron emission tomography imaging of simian immunodeficiency virus-infected rhesus macaques. Proc Natl Acad Sci U S A.
32 Reivich M., Kuhl D., Wolf A., Greenberg J., Phelps M., Ido T., Casella V., Fowler J., Hoffman E., Alavi A., Som P., Sokoloff L. (1979). The [18F]fluorodeoxyglucose method for the measurement of local cerebral glucose utilization in man. Circ Res.
33 Hawkins R.A., Mazziotta J.C., Phelps M.E., Huang S.C., Kuhl D.E., Carson R.E., Metter E.J., Riege W.H. (1983). Cerebral glucose metabolism as a function of age in man: influence of the rate constants in the fluorodeoxyglucose method. J Cereb Blood Flow Metab.
34 Heiss W.D., Pawlik G., Herholz K., Wagner R., Goldner H., Wienhard K. (1984). Regional kinetic constants and cerebral metabolic rate for glucose in normal human volunteers determined by dynamic positron emission tomography of [18F]-2-fluoro-2-deoxy-D-glucose. J Cereb Blood Flow Metab.
35 Huang S.C., Phelps M.E., Hoffman E.J., Sideris K., Selin C.J., Kuhl D.E. (1980). Noninvasive determination of local cerebral metabolic rate of glucose in man. Am J Physiol.
36 Phelps M.E., Huang S.C., Hoffman E.J., Selin C., Sokoloff L., Kuhl D.E. (1979). Tomographic measurement of local cerebral glucose metabolic rate in humans with (F-18)2-fluoro-2-deoxy-D-glucose: validation of method. Ann Neurol.
37 Jones S.C., Alavi A., Christman D., Montanez I., Wolf A.P., Reivich M. (1982). The radiation dosimetry of 2 [F-18]fluoro-2-deoxy-D-glucose in man. J Nucl Med.
38 Mejia A.A., Nakamura T., Masatoshi I., Hatazawa J., Masaki M., Watanuki S. (1991). Estimation of absorbed doses in humans due to intravenous administration of fluorine-18-fluorodeoxyglucose in PET studies. J Nucl Med.
39 Newberg A., Alavi A., Reivich M. (2002). Determination of regional cerebral function with FDG-PET imaging in neuropsychiatric disorders. Semin Nucl Med.
40 Tai Y.F., Piccini P. (2004). Applications of positron emission tomography (PET) in neurology. J Neurol Neurosurg Psychiatry.
41 Otsuka H., Graham M., Kubo A., Nishitani H. (2004). Clinical utility of FDG PET. J Med Invest.
42 Alavi A., Kung J.W., Zhuang H. (2004). Implications of PET based molecular imaging on the current and future practice of medicine. Semin Nucl Med.